# 8-((E)-4-Fluoro-but-2-enyl)-3β-p-tolyl-8-aza-bicyclo[3.2.1]octane-2β-carboxylic acid [^11^C]methyl ester

Chemical name: | 8-((E)-4-Fluoro-but-2-enyl)-3β-p-tolyl-8-aza-bicyclo[3.2.1]octane-2β-carboxylic acid [^11^C]methyl ester
Abbreviated name: | [^11^C]LBT-999
Synonym: | [^11^C]-(E)-N-(4-Fluorobut-2-enyl)-2β-carbomethoxy-3β-(4'-tolyl)nortropane
Agent category: | Compound
Target: | Dopamine transporter (DAT)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LBT-999)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in the striatum, resulting in a loss of dopamine transporters (DAT) in the presynaptic nerve terminals (1, 2). Reduction of DAT density is inversely correlated with the severity of motor dysfunction in PD patients. Several cocaine analogs were developed for the evaluation of DAT density in neurons of PD patients. Radiolabeled 2β-carboxymethoxy-3β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (3-6). Because of the short physical half-life of ^11^C-labeled analogs, equilibrium conditions are difficult to achieve in positron emission tomography (PET) measurements. [^123^I]β-CIT was studied in single-photon emission computed tomography (SPECT), which showed slow tracer uptake kinetics (7, 8). A new tropane derivative, [^11^C]-(E)-N-(4-fluorobut-2-enyl)-2β-carbomethoxy-3β-(4'-tolyl)nortropane ([^11^C]LBT-999), was evaluated as a radioligand for studies of the DAT with PET imaging (9-11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LBT-999%20AND%20synthesis)]

[^11^C]LBT-999 was synthesized with a standard methylation reaction of its corresponding carboxylic acid precursor with [^11^C]methyl triflate (10). The radiochemical yields were 19–45% (n = 10) based on [^11^C]CO_2_. The radiochemical purity was >99%, with specific activities of 30–45 GBq/µmol (0.81–1.22 Ci/µmol) at the end of synthesis. The total synthesis time was 25–30 min.

## In Vitro studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LBT-999%20AND%20in%20vitro)]

Using in vitro binding experiments on rat striatal membranes, Dolle et al. (10) showed that [^3^H]LBT-999 bound to a single site with a dissociation constant value of 9 nM and a maximal binding value of 17 pmol/mg protein, and the agent displayed a very high selectivity for the DAT. The 50% inhibition concentration (IC_50_) values were 2.4 and 18 nM for DAT-selective inhibitors GBR 12909 and PE2I, respectively. The IC_50_ values for paroxetine, citalopram, nisoxetine, and desipramine were >1 μM. Autoradiographic studies with [^3^H]LBT-999 in human post-mortem brain sections showed high radioactivity levels in the putamen and caudate, with weak binding in the thalamus and little binding in the cortical regions (9). Binding in the brain was totally blocked in the presence of 10 µM PE2I.

## Animal Studies

### Rodents

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LBT-999%20AND%20rodentia)

Chalon et al. (9) performed biodistribution studies in rats (n = 4/group) at 10, 30, and 60 min after injection of 2.22 MBq (0.06 mCi), with striatum radioactivity levels of 4.90, 4.95, and 3.37% injected dose/g (ID/g), respectively. The striatum/cerebellum radioactivity ratios were 7, 18, and 25 at 10, 30, and 60 min after injection, respectively. Weak radioactivity was observed in the cerebellum (<0.3% ID/g) and cortex (~0.6% ID/g) at 30 min after injection. Pre-administration of the DAT inhibitor GBR 12909 (5 mg/kg) inhibited the binding in the striatum by ~70%, whereas administration of paroxetine (serotonin transporter inhibitor) and nisoxetine (norepinephrine transporter inhibitor) resulted in little inhibition.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LBT-999+AND+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LBT-999%20AND%20monkeys)]

Chalon et al. (9) performed PET studies in baboons after injection of 419 MBq (11.3 mCi) [^11^C]LBT-999. The highest accumulation was observed in the putamen and caudate, with peak uptake at 40 min (16.3 and 13.3% ID/100 ml, respectively). The washout was slow (30–80 min). Radioactivity accumulation in the midbrain peaked at 12 min (6.9% ID/100 ml) and decreased with time. The lowest accumulation was observed in the cortex and cerebellum (1.37 and 1.09% ID/100 ml, respectively). The putamen/cerebellum, caudate/cerebellum, midbrain/cerebellum, thalamus/cerebellum, and cortex/cerebellum ratios were 30, 25, 6, 2, and 1, respectively. Dolles et al. (10) showed that injection of PE2I (1 mg/kg) at 80 min after injection of [^11^C]LBT-999 in a baboon inhibited the radioactivity level in the caudate, putamen, and thalamus by 74–81%. Saba et al. (11) extended the PET studies using the Logan graphical analysis (distribution volume), one-tissue compartment model (distribution volume), and simplified tissue model (binding potential). The distribution volume of the various brain regions determined with the one-tissue kinetic model was similar to those obtained using the Logan graphical analysis. The simplified tissue model using the cerebellum as a reference tissue estimated the binding potential of the putamen, caudate, midbrain, thalamus, and cortex to be 24.7, 22.4, 2.4, 0.7, and 0.1, respectively. The serotonin transporter antagonist citalopram (5 mg/kg) or the norepinephrine transporter antagonist maprotiline (5 mg/kg) had little effect on the binding potential in these brain regions. On the other hand, PE2I (1 mg/kg) induced an almost complete inhibition of the binding potential in the putamen (96%), caudate (96%), midbrain (92%), and thalamus (71%). The fraction of unchanged [^11^C]LBT-999 in plasma samples was 25% at 30 min after injection with two polar metabolites.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LBT-999%20AND%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
4 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
5 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
6 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
7 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
8 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
9 Chalon S., Hall H., Saba W., Garreau L., Dolle F., Halldin C., Emond P., Bottlaender M., Deloye J.B., Helfenbein J., Madelmont J.C., Bodard S., Mincheva Z., Besnard J.C., Guilloteau D. (2006). Pharmacological characterization of (E)-N-(4-fluorobut-2-enyl)-2beta-carbomethoxy-3beta-(4'-tolyl)nortropane (LBT-999) as a highly promising fluorinated ligand for the dopamine transporter. J Pharmacol Exp Ther.
10 Dolle F., Emond P., Mavel S., Demphel S., Hinnen F., Mincheva Z., Saba W., Valette H., Chalon S., Halldin C., Helfenbein J., Legaillard J., Madelmont J.C., Deloye J.B., Bottlaender M., Guilloteau D. (2006). Synthesis, radiosynthesis and in vivo preliminary evaluation of [11C]LBT-999, a selective radioligand for the visualisation of the dopamine transporter with PET. Bioorg Med Chem.
11 Saba W., Valette H., Schollhorn-Peyronneau M.A., Coulon C., Ottaviani M., Chalon S., Dolle F., Emond P., Halldin C., Helfenbein J., Madelmont J.C., Deloye J.B., Guilloteau D., Bottlaender M. (2007). [11C]LBT-999: a suitable radioligand for investigation of extra-striatal dopamine transporter with PET. Synapse.